# ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-LLP2A

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-LLP2A
Abbreviated name: | ^111^In-DOTA-LLP2A
Synonym:
Agent category: | Peptide
Target: | Integrin α_4_β_1_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=119631392), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=67191026) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3676) for more information about integrin α_4_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A)]

Integrins are a family of cell surface heterodimeric glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. The α_4_β_1_ integrin plays an important role in hematopoiesis of lymphocytes. On the other hand, it affects tumor growth, tumor invasiveness, and metastasis (2). The α_4_β_1_ integrin is strongly expressed on lymphoid tumor cells (3). N-[[4-[[[(2-ethylphenyl)amino]carbonyl]amino]phenyl]acetyl]-N(epsilon)-6-[(2E)-1-oxo-3-(3-pyridinyl-2-propenyl)]-L-lysyl-L-2-aminohexanedioyl-(1-amino-1-cyclohexane)carboxamide (LLP2A) was identified as a tripeptide peptidomimetic ligand to bind to α_4_β_1_ integrin on human Jurkat T-lymphoid leukemia cells using “one-bead one compound” combinatorial libraries (4). LLP2A was conjugated with Alexa Fluor 680 (Alexa680) via biotin and streptavidin (SA) interaction to study in vivo biodistribution of the tracer in tumor-bearing mice (4). LLP2A-SA-Alexa680 was found to have a high specific accumulation in α_4_β_1_-positve lymphoid tumor cells in nude mice. DeNardo et al. (5) prepared ^111^In-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-LLP2A (^111^In-DOTA-LLP2A) for use in single-photon emission computed tomography imaging of α_4_β_1_ expression in tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+synthesis)]

DOTA-LLP2A was obtained using solid-phase synthesis (5). Fmoc-Lys(Dde)-OH was first coupled to the resin, then 2 linkers were coupled to Lys(Dde). LLP2A was assembled on the N terminus of the linker. DOTA was coupled to the side chain of Lys(Dde). Radiolabeling was performed by mixing 148–185 MBq (4–5 mCi) ^111^InCl_3_ with DOTA-LLP2A. The mixture was heated in acetate buffer (pH 5.5) for 30 min at 50ºC. The radiochemical purity and specific activity of ^111^In-DOTA-LLP2A were >95% and 925 MBq/µmol (25 mCi/µmol), respectively. The labeling yield was 75–90%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+and+in+vitro)]

An in vitro receptor-binding assay of ^111^In-DOTA-LLP2A was performed on the α_4_β_1_-expressing human Raji lymphoma cell line (5). There were 1.7 × 10^5^ sites/cell with an association constant value of 2 × 10^8^ M^-1^. Binding of ^111^In-DOTA-LLP2A (1 ng/10^6^ cells) to α_4_β_1_ integrin was 25% of the incubation dose after 60 min of incubation at room temperature. Peng et al. (4) showed that LLP2A binds to α_4_β_1_, but not to α_v_β_1_, α_v_β_3_, α_3_β_1_ α_2_β_1_, α_6_β_1_, α_9_β_1_ (closely related to α_4_β_1_), α_L_β_2_ and α_M_β_2_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+rodentia)]

DeNardo et al. (5) performed ex vivo biodistribution studies of ^111^In-DOTA-LLP2A in nude mice bearing Raji subcutaneous xenografts. Images were obtained after injection of ^111^In-DOTA-LLP2A (1 nmol/mouse) at 4 and 24 h after injection. The tumor radioactivity levels were 1.2% injected dose per gram (ID/g) at 4 h and 0.8% ID/g at 24 h. The accumulation of the tracer was highest in the kidney (1.2–1.8% ID/g), followed by the marrow (0.6–0.9% ID/g) and spleen (0.3–0.8% ID/g). The radioactivity levels were low in the blood, liver, lung, muscle, and bone (<0.1% ID/g). The tumor/blood ratios were 22 at 4 h and 29 at 24 h after injection. Whole-body autoradiographic images were obtained for ^111^In-DOTA-LLP2A at 24 h after injection. Only the tumor and kidneys were clearly visualized as observed in the ex vivo studies. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+human)]

No publication is currently available.

## NIH Support

U19 113298, U24 CA110804

## References

1 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
2 Holzmann B., Gosslar U., Bittner M. (1998). alpha 4 integrins and tumor metastasis. Curr Top Microbiol Immunol.
3 Vincent A.M., Cawley J.C., Burthem J. (1996). Integrin function in chronic lymphocytic leukemia. Blood.
4 Peng L., Liu R., Marik J., Wang X., Takada Y., Lam K.S. (2006). Combinatorial chemistry identifies high-affinity peptidomimetics against alpha4beta1 integrin for in vivo tumor imaging. Nat Chem Biol.
5 Denardo S.J., Liu R., Albrecht H., Natarajan A., Sutcliffe J.L., Anderson C., Peng L., Ferdani R., Cherry S.R., Lam K.S. (2009). 111In-LLP2A-DOTA Polyethylene Glycol-Targeting {alpha}4{beta}1 Integrin: Comparative Pharmacokinetics for Imaging and Therapy of Lymphoid Malignancies. J Nucl Med.